# (1R,2R)-N-(3-(4-[^11^C]Methoxyphenyl)-4-methylisothiazol-5-yl)-2-methylcyclopropane-carboxamide

Chemical name: | (1R,2R)-N-(3-(4-[^11^C]Methoxyphenyl)-4-methylisothiazol-5-yl)-2-methylcyclopropane-carboxamide
Abbreviated name: | [^11^C]LY2428703
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LY2428703)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) radioligands targeting mGluR5 can visualize and analyze mGluR5 expression in normal physiological and pathological conditions (4-8). However, only a few mGluR1 ligands have been studied (1R, 2R). -N-(3-(4-hydroxyphenyl)-4-methylisothiazol-5-yl)-2-methylcyclopropane-carboxamide (LSN2606428) has been shown to inhibit both mGluR1 and mGluR5. Zanotti-Fregonara et al. (9) prepared (1R, 2R)-N-(3-(4-methoxyphenyl)-4-methylisothiazol-5-yl)-2-methylcyclopropane-carboxamide (LY2428703), the methoxy analog of LSN2606428, and labeled the analog as (1R, 2R)-N-(3-(4-[^11^C]methoxyphenyl)-4-methylisothiazol-5-yl)-2-methylcyclopropane-carboxamide ([^11^C]LY2428703) for use with in vivo PET imaging of mGluR1 distribution in rat brain. LY2428703 has been shown to be a full mGluR1 antagonist and partial mGluR5 antagonist.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2428703%20and%20synthesis)]

Zanotti-Fregonara et al. (9) synthesized [^11^C]LY2428703 by methylation of LNS2483097 with [^11^C]MeOTf for 5 min at 80°C. Subsequent separation with high-performance liquid chromatography produced a radiochemical purity of >99%. An average radiochemical yield was 5.4% (n = 9) based on [^11^C]CO_2_. The specific activity of [^11^C]LY2428703 was 99.3 ± 24.9 GBq/µmol (2.68 ± 0.67 Ci/µmol) at the end of synthesis. The total synthesis time was ~40 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2428703%20and%20in%20vitro)]

LY2428703 exhibited IC_50_ values of 8.9 ± 1.8 nM and 118 ± 54 nM for human mGluR1 and mGluR5, respectively, as measured with glutamine-evoked mobilization of intracellular calcium from cells expressing the mGluR (9). LNS2483097 exhibited IC_50_ values of 36.3 ± 16.5 nM and 10.2 ± 2.7 nM for human mGluR1 and mGluR5, respectively. Neither compound exhibited agonist activity for mGluR1 and mGluR5. Both agents showed IC_50_ values of >12,500 nM for mGluR2, mGluR3, mGluR4, mGluR7, and mGluR8. LY2428703 and LNS2483097 exhibited logD 7.4 values of 4.02 and 1.42, respectively. LY2428703 is more lipophilic than LNS2483097. In vitro cell-based assays showed that [^11^C]LY2428703 is not a P-glycoprotein (P-gp) substrate.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2428703%20and%20rodentia)]

Zanotti-Fregonara et al. (9) performed dynamic PET imaging studies for 90 min in rats (n = 10) after intravenous injection of 38.7 MBq (1.05 mCi) [^11^C]LY2428703 (0.7 nmol). Blocking studies were performed with pretreatment of excess mGluR1 antagonist LY2212157 (10 mg/kg, n = 4) or mGluR5 antagonist MTEP (5 mg/kg, n = 2). Baseline tissue time-activity curves revealed a high accumulation of radioactivity that peaked at 10 min in the cerebellum, with faint radioactivity in the forebrain. LY2212157 reduced the radioactivity in the cerebellum and forebrain to background level at 20 min, whereas MTEP showed little inhibition of radioactivity in the cerebellum and forebrain. Displacement studies were performed at 15 min after tracer injection. LY2212157 produced a rapid decrease in radioactivity in the cerebellum to the radioactivity level of the forebrain. Little displacement of radioactivity was observed in the forebrain. [^11^C]LY2428703 was 75%, 83%, and 96% intact in the plasma, brain, and cerebellum, respectively, at 30 min after injection. There was one major hydrophilic radiometabolite in the plasma, brain, and cerebellum. In vivo PET imaging studies showed that [^11^C]LY2428703 is not a P-glycoprotein (P-gp) substrate, as there was no difference in radioactivity levels in the cerebellum and whole brain of P-gp knockout and wild-type mice (n = 4/group).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2428703%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2428703%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=LY2428703%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and preclinical evaluation of 11C-ABP688 as a probe for imaging the metabotropic glutamate receptor subtype 5. J Nucl Med.
6 Ametamey S.M., Treyer V., Streffer J., Wyss M.T., Schmidt M., Blagoev M., Hintermann S., Auberson Y., Gasparini F., Fischer U.C., Buck A. (2007). Human PET studies of metabotropic glutamate receptor subtype 5 with 11C-ABP688. J Nucl Med.
7 Baumann C.A., Mu L., Johannsen S., Honer M., Schubiger P.A., Ametamey S.M. (2010). Structure-activity relationships of fluorinated (E)-3-((6-methylpyridin-2-yl)ethynyl)cyclohex-2-enone-O-methyloxime (ABP688) derivatives and the discovery of a high affinity analogue as a potential candidate for imaging metabotropic glutamate recepors subtype 5 (mGluR5) with positron emission tomography (PET). J Med Chem.
8 Honer M., Stoffel A., Kessler L.J., Schubiger P.A., Ametamey S.M. (2007). Radiolabeling and in vitro and in vivo evaluation of [(18)F]-FE-DABP688 as a PET radioligand for the metabotropic glutamate receptor subtype 5. Nucl Med Biol.
9 Zanotti-Fregonara P., Barth V.N., Liow J.S., Zoghbi S.S., Clark D.T., Rhoads E., Siuda E., Heinz B.A., Nisenbaum E., Dressman B., Joshi E., Luffer-Atlas D., Fisher M.J., Masters J.J., Goebl N., Kuklish S.L., Morse C., Tauscher J., Pike V.W., Innis R.B. (2013). Evaluation in vitro and in animals of a new (11)C-labeled PET radioligand for metabotropic glutamate receptors 1 in brain. Eur J Nucl Med Mol Imaging.